# Humanized anti-CD44v6 monoclonal antibody labeled with IRDye800CW

Chemical name: | Humanized anti-CD44v6 monoclonal antibody labeled with IRDye800CW
Abbreviated name: | Anti-CD44v6-IRDye800CW
Synonym:
Agent Category: | Antibody
Target: | CD44 antigen
Target Category: | Antigen
Method of detection: | Near-infrared fluorescence (NIRF); optical imaging
Source of signal / contrast: | IRDye800CW
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=CD44v6&cmd=DetailsSearch)]

The CD44 antigen, a member of the cell adhesion molecule family, is known to promote cell migration and survival during cancer metastasis (1). The mouse CD44 gene contains ~20 exons, of which 10 are variants that are alternatively spliced for incorporation into the molecule, a phenomenon that leads to the production of several CD44 variants (CD44v). The different CD44v forms have been reviewed by Ponta et al. (2). The various CD44v molecules are believed to promote cancer metastasis by modulating a variety of cellular processes that are involved in cell migration and localization in the different organs (3). Among the CD44 variants, the one that contains domain 6 of the exons (CD44v6) is specifically implicated in the tumorigenesis and migration of tumor cells during metastasis (4). The CD44v6 antigen is expressed only in a subset of normal epithelial cells, but it is found in most squamous cell carcinomas and some adenocarcinomas; CD44v6 is rarely observed in tumors with a nonepithelial origin (4). CD44v6 was reported to have higher expression than the epidermal growth factor receptor in head and neck squamous cell carcinoma (HNSCC) tumors (5). Investigators have also shown that the CD44v6 antigen is expressed in 64% of breast cancers, and thus it was suggested to be an appropriate marker for the noninvasive imaging of this cancer (6).

Because of its high expression in HNSCC, CD44v6 has been targeted with a monoclonal antibody (MAb), designated U36, for the diagnosis of this cancer in humans (7, 8). The biodistribution of ^99m^Tc-labeled U36 was investigated in patients with HNSSC, and it was shown that the labeled MAb can be used with single-photon emission computed tomography (SPECT) to detect all the primary tumors of HNSCC; however, this technique did not visualize the micro-tumors, tumor nodes with necrosis, or tumors containing keratin or fibrin (7). ^188^Re-Labeled U36 was evaluated in two clinical trials for the treatment of HNSCC, but the ^186^Re dose was insufficient to kill small tumors or to decimate single cells from this cancer (9). The use of ^211^At- and ^131^I-labeled U36 was evaluated and compared for the in vitro treatment of cells derived from HNSCC; the ^211^At-conjugated MAb was more lethal to the HNSCC cells than the ^131^I-labeled homolog (10). In addition, the ^211^At-labeled MAb was shown to stabilize or decrease the volume of HNSCC xenograft tumors in nude mice (11). Investigators labeled the U36 MAb with ^124^I or ^131^I and showed that the two tracers can be used with positron emission tomography (for ^124^I-labeled U36) or SPECT (for ^131^I-labeled U36) for the detection of xenograft tumors in nude mice (12, 13). In another study, it was shown that SPECT imaging with ^186^Re-labeled humanized anti-CD44v6 MAb can detect up to 66% of breast cancer lesions (14).

Radiolabeled small molecule compounds and MAbs are often used to detect neoplastic tumors, but these tracers are not suitable for use with image-guided surgical resection of small (and usually non-palpable) cancerous lesions of the breast, such as those observed with ductal carcinoma in situ (DCIS) (15). However, near-infrared fluorescent (NIRF) dyes conjugated to cancer-targeting molecules have been used successfully to visualize tumor boundaries during the surgical removal of cancerous tissues (16). The tumors can be visualized easily with the NIRF tracers because these agents infiltrate the tissues (17) and generate a low background in the lesions (18). On the basis of this information, the humanized anti-CD44v6 MAb was conjugated with IRDye800CW (anti-CD44v6-IRDye800CW), and the biodistribution of the NIRF dye-MAb conjugate was investigated in a mouse model of DCIS (15). The conjugate was also evaluated for the NIRF visualization of DCIS tumors in the rodents.

### Related Resource Links

CD44v6-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=CD44v6+AND+micad%5Bbook%5D&view=chapter)

Human CD44 in Gene database (http://www.ncbi.nlm.nih.gov/gene?cmd=Retrieve&dopt=full_report&list_uids=960). Gene ID: 960

CD44 in Online Mendelian Inheritance in Man databse (OMIM (http://omim.org/entry/107269))

Clinical trials (http://www.clinicaltrials.gov/ct2/results?term=CD44) related to CD44

Protein and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_001202555.1) sequences of human CD44, transcript variant 6

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-CD44v6-IRDye%20800CW%20synthesis&cmd=DetailsSearch)]

Humanized anti-CD44v6 MAb was produced and conjugated with IRDye800CW as described by Vermeulen et al. (15). The same procedure was used to produce and generate a human IgG-IRDye800CW conjugate (IRDye800CW-IgG) for use as a control (15). The IRDye800CW/anti-CD44v6 MAb and the IRDye800CW/IgG ratios were 1.43 and 1.57, respectively. The final purified preparations of the conjugates were reported to contain 5.6% free dye (15).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-CD44v6-IRDye%20800CW%20in%20vitro&cmd=DetailsSearch)]

The apparent K_d_ values of anti-CD44v6-IRDye800CW for MCF10DCIS cells (positive for CD44v6) and MDA-MB-231 cells (negative for CD44v6) were 10 nM and 17 μM, respectively, and the apparent K_d_ values of IRDye800CW-IgG (control) for these cell lines were 40 nM and 90 nM, respectively (15). The B_max_ of IRDye800CW-IgG for the MCF10DCIS cells was reported to be 13-fold smaller than that of anti-CD44v6-IRDye800CW (15).

The in vivo binding specificity of anti-CD44v6-IRDye800CW to the MCF10DCIS cell tumors was confirmed with immunohistochemical techniques as described by Vermeulen et al. (15).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-CD44v6-IRDye%20800CW%20rodentia&cmd=DetailsSearch)]

The biodistribution patterns of anti-CD44v6-IRDye800CW and IRDye800CW-IgG were studied in SCID Beige mice (C.B-17/IcrHsdPrkdc^scid^Lyst^bg^) bearing MCF10DCIS cell or MDA-MB-231 cell tumors, as described in detail elsewhere (15). The animals (n = 6 mice/tracer) were injected with ~666.7 pmol of each probe. The rodents were euthanized at 8 d postinjection (p.i.), and the organs of interest were removed to measure the NIRF signal intensity in the various tissues, including the tumors. Results were presented as percent of injected dose per gram tissue (% ID/g). With both tracers, the amount of signal generated in the blood and the normal muscle was 2% ID/g and ~0.2% ID/g, respectively. The amount of signal in the MCF10DCIS cell tumors was 9.9 ± 0.8% ID/g and 2.8 ± 0.2% ID/g with anti-CD44v6-IRDye800CW and IRDye800CW-IgG, respectively. In the MDA-MB-231 cell tumors, the accumulation of dye with anti-CD44v6-IRDye800CW and IRDye800CW-IgG was 2.9 ± 0.5% ID/g and 2.5 ± 0.3% ID/g, respectively. All other organs (liver, kidney, and spleen) showed an accumulation between 1.5% ID/g and 2.0% ID/g. This indicated that the NIRF signal generated with anti-CD44v6-IRDye800CW in the MCF10DCIS cell tumors can be used to detect cancerous lesions that express high levels of CD44v6 in rodents. No blocking studies were reported.

The anti-CD44v6-IRDye800CW and IRDye800CW-IgG conjugates were evaluated for the noninvasive imaging of MCF10DCIS cell tumors and MDA-MB-231 cell tumors in mice (15). The rodents (n = 6 mice/time point per tracer) were injected with the tracers as before, and whole-body NIRF images of the anesthetized mice were acquired at various time points ranging from 4 h p.i. to 192 h (8 d) p.i. At 4 h p.i., the NIRF signals were detectable in the MCF10DCIS cell tumors of mice injected with anti-CD44v6-IRDye800CW, but no signal was generated from these tumors in mice treated with IRDye800CW-IgG. With anti-CD44v6-IRDye800CW, the maximum fluorescence intensity (~7,000 counts/s) was obtained at 24 h p.i. from the MCF10DCIS cell lesions; this intensity decreased to ~3,500 counts/s by 5 d p.i. and remained relatively constant up to 8 d p.i. With IRDye800CW-IgG, the maximum fluorescence intensity in the MCF10DCIS cell tumors was observed at 8 h p.i. (~5,500 counts/s) and showed a constant decline up to 8 d p.i. (~1,750 counts/s). With anti-CD44v6-IRDye800CW, the MCF10DCIS cell tumor/background ratio was 2.41 ± 0.39 at 3 d p.i., and this ratio showed a consistent increase to 2.78 ± 0.31 up to 7 d p.i. With IRDye800CW-IgG, the MCF10DCIS cell tumor/background ratio was a maximum of ~1.75 at 3 d p.i., decreased to ~1.3 at 8 d p.i., and was significantly lower (P = 0.004) than the ratio obtained with anti-CD44v6-IRDye800CW. Both tracers had a comparable tumor/background ratio with the MDA-MB-231 cell lesions (~1.40, P = 0.201), and this was significantly lower than the ratio obtained with the MCF10DCIS tumors (P = 0.011). No blocking studies were reported.

From these studies, the investigators concluded that anti-CD44v6-IRDye800CW can probably be used with NIRF imaging techniques for the detection of DCIS lesions in rodents (15).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-CD44v6-IRDye%20800CW%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-CD44v6-IRDye%20800CW%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-CD44v6-IRDye%20800CW%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Naor D., Wallach-Dayan S.B., Zahalka M.A., Sionov R.V. (2008). Involvement of CD44, a molecule with a thousand faces, in cancer dissemination. Semin Cancer Biol.
2 Ponta H., Sherman L., Herrlich P.A. (2003). CD44: from adhesion molecules to signalling regulators. Nat Rev Mol Cell Biol.
3 Wallach-Dayan S.B., Rubinstein A.M., Hand C., Breuer R., Naor D. (2008). DNA vaccination with CD44 variant isoform reduces mammary tumor local growth and lung metastasis. Mol Cancer Ther.
4 Heider K.H., Kuthan H., Stehle G., Munzert G. (2004). CD44v6: a target for antibody-based cancer therapy. Cancer Immunol Immunother.
5 Nestor M., Ekberg T., Dring J., van Dongen G.A., Wester K., Tolmachev V., Anniko M. (2007). Quantification of CD44v6 and EGFR expression in head and neck squamous cell carcinomas using a single-dose radioimmunoassay. Tumour Biol.
6 Vermeulen J.F., van Brussel A.S., van der Groep P., Morsink F.H., Bult P., van der Wall E., van Diest P.J. (2012). Immunophenotyping invasive breast cancer: paving the road for molecular imaging. BMC Cancer.
7 de Bree R., Roos J.C., Quak J.J., den Hollander W., Snow G.B., van Dongen G.A. (1995). Radioimmunoscintigraphy and biodistribution of technetium-99m-labeled monoclonal antibody U36 in patients with head and neck cancer. Clin Cancer Res.
8 de Bree R., Roos J.C., Plaizier M.A., Quak J.J., van Kamp G.J., den Hollander W., Snow G.B., van Dongen G.A. (1997). Selection of monoclonal antibody E48 IgG or U36 IgG for adjuvant radioimmunotherapy in head and neck cancer patients. Br J Cancer.
9 Colnot D.R., Quak J.J., Roos J.C., van Lingen A., Wilhelm A.J., van Kamp G.J., Huijgens P.C., Snow G.B., van Dongen G.A. (2000). Phase I therapy study of 186Re-labeled chimeric monoclonal antibody U36 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
10 Nestor M., Persson M., van Dongen G.A., Jensen H.J., Lundqvist H., Anniko M., Tolmachev V. (2005). In vitro evaluation of the astatinated chimeric monoclonal antibody U36, a potential candidate for treatment of head and neck squamous cell carcinoma. Eur J Nucl Med Mol Imaging.
11 Cheng J., Ekberg T., Engstrom M., Nestor M., Jensen H.J., Tolmachev V., Anniko M. (2007). Radioimmunotherapy with astatine-211 using chimeric monoclonal antibody U36 in head and neck squamous cell carcinoma. Laryngoscope.
12 Verel I., Visser G.W., Vosjan M.J., Finn R., Boellaard R., van Dongen G.A. (2004). High-quality 124I-labelled monoclonal antibodies for use as PET scouting agents prior to 131I-radioimmunotherapy. Eur J Nucl Med Mol Imaging.
13 Fortin M.A., Salnikov A.V., Nestor M., Heldin N.E., Rubin K., Lundqvist H. (2007). Immuno-PET of undifferentiated thyroid carcinoma with radioiodine-labelled antibody cMAb U36: application to antibody tumour uptake studies. Eur J Nucl Med Mol Imaging.
14 Koppe M., Schaijk F., Roos J., Leeuwen P., Heider K.H., Kuthan H., Bleichrodt R. (2004). Safety, pharmacokinetics, immunogenicity, and biodistribution of (186)Re-labeled humanized monoclonal antibody BIWA 4 (Bivatuzumab) in patients with early-stage breast cancer. Cancer Biother Radiopharm.
15 Vermeulen J.F., van Brussel A.S., Adams A., Mali W.P., van der Wall E., van Diest P.J., Derksen P.W. (2013). Near-Infrared Fluorescence Molecular Imaging of Ductal Carcinoma In Situ with CD44v6-Specific Antibodies in Mice: A Preclinical Study. Mol Imaging Biol.
16 Stroud M.R., Hansen S.J., Olson J.M. (2011). In vivo bio-imaging using chlorotoxin-based conjugates. Curr Pharm Des.
17 Frangioni J.V. (2008). New technologies for human cancer imaging. J Clin Oncol.
18 Frangioni J.V. (2003). In vivo near-infrared fluorescence imaging. Curr Opin Chem Biol.